# (+/-)-2-(N-Phenethyl-N-1'-[^11^C]propyl)amino-5-hydroxytetralin

Chemical name: | (+/-)-2-(N-Phenethyl-N-1'-[^11^C]propyl)amino-5-hydroxytetralin
Abbreviated name: | [^11^C]PPHT
Synonym:
Agent Category: | Compound
Target: | D_2_ dopamine receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five dopamine receptor subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_). D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. Most striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein–coupled receptors that exist in high- and low-affinity states with respect to agonist binding. The two states are inter-convertible. In the high-affinity state, dopamine receptors are coupled to G-proteins, whereas in the low-affinity state they are not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiologic conditions, dopamine binds predominately to receptors in the high-affinity state. The high-affinity state was suggested to be the functional form of the dopamine receptors (6).

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making study of extrastriatal D_2_ receptors difficult (7-9). In binding studies, [^123^I]epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (10). Epidepride exhibits marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective high-affinity antagonist of D_2/3_ receptors (11), and in positron emission tomography (PET) in vivo studies (12-14) it identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguishes between the high- and low-affinity states of the D_2_ receptors. (–)-N-[^11^C]Propyl-norapomorphine ([^11^C]NPA) and [^11^C](+)-4-N-propyl-,3,4a,5,6,10b-hexahydro-2H-naphth[1,2-b][1,4]oxazin-9-ol ([^11^C](+)-PHNO) have been developed as radiolabeled dopamine agonists for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain.

Various hydroxytetralin analogs with different binding affinities for the D_2_ receptors have been developed as agonist radiotracers (15). (+/-)-2-(N-Phenethyl-N-1’-[^11^C]propyl)amino-5-hydroxytetralin ([^11^C]PPHT) is being evaluated as a PET agent for the high-affinity state of D_2/3_ receptors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT%20and%20synthesis)]

Shi et al. (15) reported a two-step synthesis of [^11^C]PPHT in which [^11^C]propionyl chloride was reacted with 5-hydroxy-2-[N-(2-phenethyl)amino]tetralin and followed by LiAlH_4_ reduction, with a radiochemical yield of 5–10% (based on [^11^C]CO_2_ at the end of bombardment) and an average specific activity of 9–37 GBq/μmol (250–1,000 mCi/μmol) at end of synthesis after purification by high-performance liquid chromatography. [^11^C]Propionyl chloride was prepared by reacting [^11^C]CO_2_ with ethylmagnesium bromide, followed by reaction with phthaloyl chloride. Total synthesis time was 60–75 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT%20and%20in%20vitro)]

In a binding study of dopamine receptors in membranes of the rat striatum with [^3^H]spiperone, PPHT had an IC_50_ of 0.65 nM (15). In vitro autoradiography studies of rat brain slices indicated selective binding of [^11^C]PPHT to the striata, which was completely inhibited by co-incubation with 10 μM sulpiride. Gpp(NH)p decreased the striatum/cerebellum ratio from 2.0 to 1.1 by converting the high-affinity state to the low-affinity state. There was significant nonspecific binding in the cortex.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT%20and%20rodentia)]

Biodistribution studies in rats showed a marked accumulation of the tracer in the striata within the first 2 min [1.2% injected dose per gram (ID/g)], followed by a decrease of radioactivity to 0.5% ID/g at 30 min and 0.2% ID/g at 60 min (16). The striatum/cerebellum ratios were 1.27 at 2 min, 1.52 at 30 min, and 1.42 at 60 min after injection. Haloperidol pretreatment (1 mg/kg, 15 min before radiotracer injection) effectively reduced specific binding of [^11^C]PPHT to the striatum with some residual binding relative to the cerebellum at 30 min. Little inhibition was seen in the cerebellum. [^11^C]PPHT thus displays uptake and washout kinetics characteristic of reversible radiotracers.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT%20and%20monkey)]

Mukherjee et al. (16) showed selective accumulation (0.03% ID/ml) in the striata of two rhesus monkeys with striatum/cerebellum ratios of 1.5 at 30 min and 1.4 at 60 min after injection of 26–93 MBq (0.7–2.5 mCi) of [^11^C]PPHT. Thalamus/cerebellum ratios were 1.3 at 30 min and 1.2 at 60 min. However, there was a substantial nonspecific binding in the cortex and cerebellum. The authors suggested that the use of the more active S-isomer may provide higher striatum/cerebellum and thalamus/cerebellum ratios.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PPHT%20and%20human)]

No relevant publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Sunahara R.K., Guan H.C., O'Dowd B.F., Seeman P., Laurier L.G., Ng G., George S.R., Torchia J., Van Tol H.H., Niznik H.B. (1991). Cloning of the gene for a human dopamine D5 receptor with higher affinity for dopamine than D1. Nature.
6 Sibley D.R., De Lean A., Creese I. (1982). Anterior pituitary dopamine receptors. Demonstration of interconvertible high and low affinity states of the D-2 dopamine receptor. J Biol Chem.
7 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
8 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
9 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
10 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
11 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
12 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2005). and , The Striatal and Extrastriatal D2/D3 Receptor-Binding Profile of Clozapine in Patients with Schizophrenia. Neuropsychopharmacology.
13 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
14 Kessler R.M., Ansari M.S., Riccardi P., Li R., Jayathilake K., Dawant B., Meltzer H.Y. (2005). Occupancy of striatal and extrastriatal dopamine d(2)/d(3) receptors by olanzapine and haloperidol. Neuropsychopharmacology.
15 Shi B., Narayanan T.K., Yang Z.Y., Christian B.T., Mukherjee J. (1999). Radiosynthesis and in vitro evaluation of 2-(N-alkyl-N-1'-11C-propyl)amino-5-hydroxytetralin analogs as high affinity agonists for dopamine D-2 receptors. Nucl Med Biol.
16 Mukherjee J., Narayanan T.K., Christian B.T., Shi B., Yang Z.Y. (2004). Binding characteristics of high-affinity dopamine D2/D3 receptor agonists, 11C-PPHT and 11C-ZYY-339 in rodents and imaging in non-human primates by PET. Synapse.